# ^111^In-DOTA-Gly-benzoyl-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_

Chemical name: | ^111^In-DOTA-Gly-benzoyl-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_
Abbreviated name: | ^111^In-RM1
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal\contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM1)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (2). Specific BBN receptors (BBN-R) have been identified on CNS and GI tissuesincluding the pancreas and on a number of tumor cell lines. The BBN-R superfamily includes at least four different subtypes, namely neuromedin B (NMB or BB1), the GRPR subtype (BB2), the BB3 subtype, and the BB4 subtype (3). The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR.

Currently used targeting GRPR peptides mainly are agonists. Therefore, there is a need for GRPR antagonist radioligands. Llinares et al. (4) has developed a series of GRPR peptide antagonists. One of them, D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM26), was found to be a selective GRPR antagonist. DOTA-Gly-benzoyl group was added to the C-terminus to form DOTA-Gly-benzoyl-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM1). For evaluation as a single-photon emission computed tomography (SPECT) imaging agent for GRPR, ^111^In has been attached to RM1 to form ^111^In-RM1 (5).

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=GRPR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925)).
- Articles in OMIM (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=Gastrin-releasing+peptide+receptor+))
- Drug information in FDA (GRPR (http://google-test.fda.gov/search?q=GASTRIN-RELEASING+PEPTIDE+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM1+synthesis)]

RM1 was prepared by solid-phase peptide synthesis with a 30% yield (5). ^111^InCl_3_ was added to a solution of RM1 (~6 nmol) in sodium acetate (pH 5). The mixture was heated for 30 min at 95°C. The product, ^111^In-RM1, was identified with electrospray-mass spectrometry and used without further purification. The labeling yield of ^111^In-RM1 was >95% with a specific activity of 30 GBq/µmol (0.81 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM1+in+vitro)]

Mansi et al. (5) performed in vitro inhibition studies of RM26, RM1 and ^nat^In-RM1 in cultured PC-3 human prostate cells with ^125^I-BBN with the 50% inhibition concentration (IC_50_) values of 5.6 ± 1.8, 35.0 ± 13.0, and 14.0 ± 3.4 nM, respectively. The GRPR agonist, ^nat^Lu-AMBA, showed the IC_50_ value of 0.8 ± 0.1 nM. ^111^In-RM1 showed a K_d_ (affinity constant) of 8.5 ± 2.7 nM and a B_max_ (receptor density) of 2.4 ± 0.2 nM, whereas ^111^Lu-AMBA showed a higher affinity (K_d_, 0.6 ± 0.3 nM) but a lower receptor density (B_max_, 0.7 ± 0.1 nM). PC-3 cells exhibited a 4.7% uptake of incubation dose (ID) of ^111^In-RM1 inside the cells at 4 h of incubation at 37°C with 21.8% of ID remained on the cell surface, indicating a lack of cell internalization of the radioligand. Only 10% of the internalized radioactivity remained inside the cells over 4 h of incubation in fresh medium. On the other hand, 29% of ID of ^111^Lu-AMBA was inside the cells with 4.3% of ID on the cell surface. About 40% of the internalized radioactivity remained inside the cells over 4 h of incubation in fresh medium. ^nat^In-RM1 was able to inhibit the calcium release and receptor internalization induced by BBN.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM1+rodentia)]

Mansi et al. (5) performed ex vivo biodistribution studies of 0.18 MBq (5 μCi) ^111^In-RM1 or ^111^Lu-AMBA in nude mice bearing PC-3 tumors. Tumor accumulation for ^111^In-RM1 was 14.2 ± 1.8, 13.5 ± 0.8, and 6.6 ± 1.1% ID/g at 1, 4, and 24 h after injection, respectively. Tumor accumulation for ^111^Lu-AMBA was 4.5 ± 0.7, 3.7 ± 0.8, and 3.0 ± 0.6% ID/g at 1, 4, and 24 h after injection, respectively. Both tracers exhibited a fast blood clearance with 0.05% ID/g at 4 h after injection. The tumor/blood ratios were 17, 336, and 658 for ^111^In-RM1 and 14, 74, and 147 for ^111^Lu-AMBA at 1, 4, and 24 h after injection, respectively. Preinjection of excess cold peptide (20 nmol, 5 min) inhibited the tumor, pancreas, small intestine, and large intestine accumulation by ~90% with little effect in the other tissues at 4 h after tracer injection. ^111^In-RM1 exhibited a faster washout from most of the normal organs and tissues than ^111^Lu-AMBA. SPECT imaging in nude mice bearing PC-3 xenografts was performed with 4 MBq (0.11 mCi) ^111^In-RM1 at 4, 24, 48 and 72 h after injection. The tumors were clearly visualized at these time points. Pretreatment with excess RM1 (20 nmol, 15 min) completely inhibit the accumulation of radioactivity in the tumor at 4 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM1+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM1+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM1+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
3 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
4 Llinares M., Devin C., Chaloin O., Azay J., Noel-Artis A.M., Bernad N., Fehrentz J.A., Martinez J. (1999). Syntheses and biological activities of potent bombesin receptor antagonists. J Pept Res.
5 Mansi R., Wang X., Forrer F., Kneifel S., Tamma M.L., Waser B., Cescato R., Reubi J.C., Maecke H.R. (2009). Evaluation of a 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-conjugated bombesin-based radioantagonist for the labeling with single-photon emission computed tomography, positron emission tomography, and therapeutic radionuclides. Clin Cancer Res.